# Near-infrared Dye^®^800CW–conjugated disulfide-based cyclic RGD peptide c(CRGDKGPDC) and its DOTA analog

Chemical name: | Near-infrared Dye^®^800CW–conjugated disulfide-based cyclic RGD peptide c(CRGDKGPDC) and its DOTA analog
Abbreviated name: | Ac-Cys(IRDye^®^800CW)-iRGD and DOTA-Cys(IRDye^®^800CW)-iRGD
Synonym:
Agent Category: | Compound
Target: | Integrin and neutrophilin-1 receptors
Target Category: | Receptors
Method of detection: | Optical imaging
Source of signal / contrast: | Near-infrared dye^®^800CW
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://ac.els-cdn.com/S1535610809003821/1-s2.0-S1535610809003821-main.pdf?_tid=12266b5f455014167496f425ac0052db&acdnat=1344354384_e3a4c56026e4c98a3a716e4b16fec1dd)]

Integrins are multifunctional cell-surface receptors that are implicated in the regulation of cell–cell interactions, angiogenesis, tumor growth, and cancer metastasis (1, 2). There are 24 known integrin receptors, and each receptor is made up by the combination of a single α subunit (with 18 subtypes) and a single β subunit (with 8 subtypes) (3). A characteristic feature of the integrin receptors is that they can be activated either by cytoplasmic events ("inside-out" activation) or by extracellular ligand binding ("outside-in" activation) as illustrated by Margadant et al. (3). Integrins such as α_v_β_3_, α_v_β_5_, and α_5_β_1_ are overexpressed in certain malignant tumors and are targeted with imaging agents for the detection, diagnosis, and therapy of cancers or to evaluate the efficacy of new anticancer agents (1). Peptides containing an arginine-glycine-aspartic acid (RGD) motif (RGD peptides) are known to recognize and bind to the integrin receptors, and a variety of radiolabeled cyclic analogs of the RGD peptides (e.g., c(RGDfk)) have been used for the molecular imaging and therapy of neoplastic tumors in the clinic (4). A disulfide-based cyclic RGD peptide, c(CRGDKGPDC) (iRGD), which interacts with the integrin and neurophilin-1 receptors, was shown to facilitate deeper penetration of imaging agents (5) and anticancer drugs (6) compared with the original RGD peptide. The complete mechanism of action of iRGD has been described and illustrated by Sugahara et al. (5). On the basis of this information, two cysteine-containing analogs of iRGD were conjugated to IRDye^®^800CW, a near-infrared dye (Cys(IRDye^®^800CW)iRGD), to generate probes that could potentially be used to detect tumors that overexpress integrins with optical imaging (1). The first peptide was an acylated form of the peptide (Ac-Cys(IRDye^®^800CW)iRGD), and the second peptide was its 1,4,7,10-tetra-azacyclodecane-N,N',N'',N'''-tetraacetic acid (DOTA) analog (DOTA-Cys(IRDye^®^800CW)iRGD) that could be used for dual labeling of the peptide. The purpose of introducing a DOTA moiety in the peptide was to generate an iRGD-based peptide that can be used for the imaging of tumors with optical and/or positron emission tomography (PET) techniques because DOTA can conjugate radionuclides such as ^64^Cu that emits positrons that can be detected with PET. The two peptides were evaluated for the optical imaging of MDA-MB-435 cell (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-129&Template=cellBiology) xenograft tumors that overexpress integrins in nude mice (1).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Integrin+receptors+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Integrin alpha V in Gene database (http://www.ncbi.nlm.nih.gov/gene/3685), Gene ID: 3685

Homo sapiens integrin beta 3, protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_000212.2) sequences

Integrin beta 3 in Gene database (http://www.ncbi.nlm.nih.gov/gene/374209), Gene ID: 374209

Clinical trials (http://clinicaltrials.gov/ct2/results?term=integrins) involving integrins

Integrins in Online Mendelian Inheritance in Man (OMIM (http://www.ncbi.nlm.nih.gov/omim?term=integrin%20)) database

Integrin signaling pathways in Pathway Interaction Database (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=100123&pathway_name=integrin%20signaling%20pathway&source=BioCarta%20Imported&what=graphic&jpg=on&ppage=1)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ac-Cys%28IRDye800CW%29iRGD%20synthesis&cmd=DetailsSearch)]

The synthesis of Ac-Cys(IRDye^®^800CW)iRGD and DOTA-Cys(IRDye^®^800CW)iRGD has been described by Ye et al. (1). The DOTA moiety on DOTA-Cys(IRDye^®^800CW)iRGD is located on the N-terminus of the peptide. The final products were purified with high-performance liquid chromatography (HPLC), and the final yields of Ac-Cys(IRDye^®^800CW)iRGD and DOTA-Cys(IRDye^®^800CW)iRGD were 20% and 30%, respectively. The identity of the peptides was confirmed with HPLC and liquid chromatography-mass spectrometry. For in vivo studies, the compounds were dissolved in phosphate-buffered saline (pH 7.2) before use.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ac-Cys%28IRDye800CW%29iRGD%20in%20vitro&cmd=DetailsSearch)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ac-Cys%28IRDye800CW%29iRGD%20rodentia&cmd=DetailsSearch)]

To confirm the tumor-targeting specificity of the peptides, nude mice bearing MDA-MB-435 cell xenograft tumors (under anesthesia; n = 3 animals/peptide) were injected with 10 μM either Ac-Cys(IRDye^®^800CW)iRGD or DOTA-Cys(IRDye^®^800CW)iRGD through the tail vein as detailed by Ye et al. (1). Near-infrared fluorescence images of the rodents were acquired at various time points ranging from 5 min postinjection (p.i.) to 240 min p.i., and the images were normalized for analysis using appropriate software. Regions of interest were drawn on the tumors and the muscles to generate tumor signal curves and to calculate the tumor/muscle (T/M) ratios at the different time points. From the signal curves it was clear that uptake of both probes by the tumors peaked at 10 min p.i. and decreased thereafter for up to 240 min p.i. The T/M ratio had a maximum of ~2.0 at 1 h p.i. and stayed relatively constant for up to 2 h p.i. Blocking studies to determine specificity of the probes were not reported.

From this study, the investigators concluded that iRGD can be used to develop imaging probes for the detection of cancerous tumors that overexpress integrins in rodents (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ac-Cys%28IRDye800CW%29iRGD%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ac-Cys%28IRDye800CW%29iRGD%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ac-Cys%28IRDye800CW%29iRGD%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Supported by National Institute Biomedical Imaging and Bioengineering, National Institutes of Health, research.

## References

1 Ye Y., Zhu L., Ma Y., Niu G., Chen X. (2011). Synthesis and evaluation of new iRGD peptide analogs for tumor optical imaging. Bioorg Med Chem Lett.
2 Ye F., Kim C., Ginsberg M.H. (2012). Reconstruction of integrin activation. Blood.
3 Margadant C., Monsuur H.N., Norman J.C., Sonnenberg A. (2011). Mechanisms of integrin activation and trafficking. Curr Opin Cell Biol.
4 Gaertner F.C., Kessler H., Wester H.J., Schwaiger M., Beer A.J. (2012). Radiolabelled RGD peptides for imaging and therapy. Eur J Nucl Med Mol Imaging.
5 Sugahara K.N., Teesalu T., Karmali P.P., Kotamraju V.R., Agemy L., Girard O.M., Hanahan D., Mattrey R.F., Ruoslahti E. (2009). Tissue-penetrating delivery of compounds and nanoparticles into tumors. Cancer Cell.
6 Sugahara K.N., Teesalu T., Karmali P.P., Kotamraju V.R., Agemy L., Greenwald D.R., Ruoslahti E. (2010). Coadministration of a tumor-penetrating peptide enhances the efficacy of cancer drugs. Science.